# Anti-α-Fetoprotein antibody-quantum dots

Chemical name: | Anti-α-Fetoprotein antibody-quantum dots
Abbreviated name: | Anti-AFP-QDs
Synonym:
Agent category: | Antibody
Target: | α-Fetoprotein (AFP)
Target category: | Antigen
Method of detection: | Optical, near-infrared (NIR)
Source of signal\contrast: | Quantum dot
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=119626086), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=4501988) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=174) for more information about AFP.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Quantum%20dot%20and%20AFP)]

Fluorescent semiconductor quantum dots (QDs) are nanocrystals made of CdSe/CdTe-ZnS with radii of 1–10 nm (1-3). They can be tuned to emit in a range of wavelengths by changing their sizes and composition, thus providing broad excitation profiles and high absorption coefficients. They have narrow and symmetric emission spectra with long excited-state lifetimes of 20–50 ns, versus 1–10 ns for fluorescent dyes. QDs possess good quantum yields of 40–90% and high extinction coefficients, and they are more photo-stable than conventional organic dyes. QDs can be coated and capped with hydrophilic materials for additional conjugation with biomolecules such as peptides, antibodies, nucleic acids, and small organic compounds, which were tested in vitro and in vivo (3-7). Although many cells have been labeled with QDs in vitro with little cytotoxicity, there are limited studies of long-term QD toxicity in small animals (8-16). However, little is known about the toxicity or the mechanisms of clearance and metabolism of QDs in humans.

α-Fetoprotein (AFP) is a single-chain glycoprotein (70 kDa) that is highly expressed in the fetal liver, gastrointestinal tract, and yolk sac (17); serum AFP levels are markedly low (<3 ng/ml) in healthy adults. Synthesis of AFP in adults appears in a variety of disease states, often associated with increased concentrations of AFP in serum. Markedly high serum levels are found in cancer patients with hepatoblastomas, nephroblastomas, hepatocellular carcinomas (HCC), and certain testicular tumors. Yu et al. (18, 19) prepared QDs conjugated with anti-AFP monoclonal antibodies to detect accumulation and retention of AFP at the site of HCC tumors. Anti-AFP-QDs are being studied as a contrast agent for imaging AFP expression in HCC cancer cells.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Quantum%20dot%20and%20AFP%20and%20synthesis)]

CdSe-ZnS QDs (with emission peaks at 590 nm) modified with thioglycolic acid were activated with 50 mmol 1-(3-dimethyl-aminopropyl)-3-ethylcarbodiimide and 5 mmol N-hydroxysuccinimide in phosphate-buffered saline (18). Mouse anti-human monoclonal AFP antibody was incubated with the activated QDs at room temperature for 2–4 h. The anti-AFP-QDs were isolated with centrifugation and purified with dialysis. The assembled anti-AFP-QDs have a spherical diameter of 5 nm, as measured with low-temperature transmission electron microscopy. The number of copies of antibody per QD was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Quantum%20dot%20and%20AFP%20and%20in%20vitro)]

Anti-AFP-QDs were examined for their ability to discriminate between the AFP-expressing HCC cell line HCCLM6 and the AFP-negative human colon cell line SW480 (20). In vitro imaging showed that anti-AFP-QDs (100 nM) could bind to HCCLM6 cells after 4 h of incubation but not to SW480 cells. Furthermore, anti-AFP-QDs (100 nM) exerted little effect on cell viability in culture for 48 h.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Quantum%20dot%20and%20AFP%20and%20rodentia)]

Chen et al. (20) performed ex vivo biodistribution studies of anti-AFP-QDs (200 nmol/kg) administered to normal mice (n = 5) via intravenous injection. The plasma half-life of anti-AFP-QDs was ~2 h. The tissue with the highest Cd (measured with inductively coupled plasma-mass-spectrometry) accumulation at 24 h was the spleen (~10% µg/g tissue), followed by the liver (~7% µg/g tissue) and kidneys (~2% µg/g tissue). There was minimal accumulation in the brain, heart, muscle, and lung. Anti-AFP-QDs were taken up by the reticuloendothelial system and by phagocytes in the liver and spleen. The mice showed no acute toxicity when compared with mice injected with saline. No signs of sickness were observed in the mice for up to 7 days after injection. Whole-body imaging of mice bearing HCCLM6 tumors and small-cell lung metastases showed a good near-infrared fluorescence signal in the tumor and lung metastases, with approximately four-fold enhancement as compared with saline injection. The near-infrared fluorescence signal was localized to both primary and metastatic tumor cells as confirmed with staining and confocal microscopy. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Quantum%20dot%20and%20AFP%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Quantum%20dot%20and%20AFP%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Quantum%20dot%20and%20AFP%20and%20human%20not%20animal%20not%20cell%20line)]

No publication is currently available.

## References

1 Chan W.C., Maxwell D.J., Gao X., Bailey R.E., Han M., Nie S. (2002). Luminescent quantum dots for multiplexed biological detection and imaging. Curr Opin Biotechnol.
2 Gao X., Nie S. (2005). Quantum dot-encoded beads. Methods Mol Biol.
3 Michalet X., Pinaud F.F., Bentolila L.A., Tsay J.M., Doose S., Li J.J., Sundaresan G., Wu A.M., Gambhir S.S., Weiss S. (2005). Quantum dots for live cells, in vivo imaging, and diagnostics. Science.
4 Alivisatos A.P., Gu W., Larabell C. (2005). Quantum dots as cellular probes. Annu Rev Biomed Eng.
5 Hilger I., Leistner Y., Berndt A., Fritsche C., Haas K.M., Kosmehl H., Kaiser W.A. (2004). Near-infrared fluorescence imaging of HER-2 protein over-expression in tumour cells. Eur Radiol.
6 Medintz I.L., Uyeda H.T., Goldman E.R., Mattoussi H. (2005). Quantum dot bioconjugates for imaging, labelling and sensing. Nat Mater.
7 Smith A.M., Gao X., Nie S. (2004). Quantum dot nanocrystals for in vivo molecular and cellular imaging. Photochem Photobiol.
8 Akerman M.E., Chan W.C., Laakkonen P., Bhatia S.N., Ruoslahti E. (2002). Nanocrystal targeting in vivo. Proc Natl Acad Sci U S A.
9 Braydich-Stolle L., Hussain S., Schlager J.J., Hofmann M.C. (2005). In vitro cytotoxicity of nanoparticles in mammalian germline stem cells. Toxicol Sci.
10 Frangioni J.V., Hajjar R.J. (2004). In vivo tracking of stem cells for clinical trials in cardiovascular disease. Circulation.
11 Gao X., Cui Y., Levenson R.M., Chung L.W., Nie S. (2004). In vivo cancer targeting and imaging with semiconductor quantum dots. Nat Biotechnol.
12 Han M., Gao X., Su J.Z., Nie S. (2001). Quantum-dot-tagged microbeads for multiplexed optical coding of biomolecules. Nat Biotechnol.
13 Lovric J., Bazzi H.S., Cuie Y., Fortin G.R., Winnik F.M., Maysinger D. (2005). Differences in subcellular distribution and toxicity of green and red emitting CdTe quantum dots. J Mol Med.
14 Ohnishi S., Lomnes S.J., Laurence R.G., Gogbashian A., Mariani G., Frangioni J.V. (2005). Organic alternatives to quantum dots for intraoperative near-infrared fluorescent sentinel lymph node mapping. Mol Imaging.
15 Shiohara A., Hoshino A., Hanaki K., Suzuki K., Yamamoto K. (2004). On the cyto-toxicity caused by quantum dots. Microbiol Immunol.
16 Soltesz E.G., Kim S., Laurence R.G., DeGrand A.M., Parungo C.P., Dor D.M., Cohn L.H., Bawendi M.G., Frangioni J.V., Mihaljevic T. (2005). Intraoperative sentinel lymph node mapping of the lung using near-infrared fluorescent quantum dots. Ann Thorac Surg.
17 Smith C.J., Kelleher P.C. (1980). Alpha-fetoprotein molecular heterogeneity. Physiologic correlations with normal growth, carcinogenesis and tumor growth. Biochim Biophys Acta.
18 Yu X., Chen L., Deng Y., Li K., Wang Q., Li Y., Xiao S., Zhou L., Luo X., Liu J., Pang D. (2007). Fluorescence analysis with quantum dot probes for hepatoma under one- and two-photon excitation. J Fluoresc.
19 Yu X., Chen L., Li K., Li Y., Xiao S., Luo X., Liu J., Zhou L., Deng Y., Pang D., Wang Q. (2007). Immunofluorescence detection with quantum dot bioconjugates for hepatoma in vivo. J Biomed Opt.
20 Chen L.D., Liu J., Yu X.F., He M., Pei X.F., Tang Z.Y., Wang Q.Q., Pang D.W., Li Y. (2008). The biocompatibility of quantum dot probes used for the targeted imaging of hepatocellular carcinoma metastasis. Biomaterials.